# ^131^I-Labeled anti-α folate receptor human antibody fragment AFRA-DMF5.3 dimer

Chemical name: | ^131^I-Labeled anti-α folate receptor human antibody fragment AFRA-DMF5.3 dimer
Abbreviated name: | [^131^I]-AFRA-DFM5.3
Synonym:
Agent Category: | Antibody
Target: | α Folate receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22SUBSTANCENAME%22%5BSubstance%5D%20AND%20Background%5BAll%20Fields%5D&cmd=DetailsSearch)]

Folic acid (FA; also known as folate or vitamin B_9_) is a water-soluble vitamin that is essential for the synthesis and repair of cellular DNA. FA also acts as a cofactor for many biological reactions and has an important role in cell maintenance and proliferation. The folate molecule is transported into the cell by the folate receptor (FR; there are two types, α and β), which is a well-investigated member of the FR family. The FRα is a ~40-kDa molecule that is fastened to the cell membrane surface via a glycophosphatidylinositol linkage and facilitates the transport of folate through endocytosis (1). Most tissues have little to no expression of the FRα, but it is expressed at measurable levels in the epithelial cells of the lungs, kidneys, and choroid plexus of the brain. However, the malignant tumors of these tissues overexpress the FRα in order to meet the increased demand for FA, which is required to synthesize cellular DNA due to the increased rate of cell proliferation (1). Therefore, the FRα is perceived to be an excellent target for the imaging and therapy of the various cancers, including that of the ovaries (2).

Most cancers tend to metastasize and are often treated with antibody (Ab)-based therapies (such as immunotherapy and/or radioimmunotherapy) that target a specific receptor (see Table 1 in Julien et al. (3) for details), but the main limitation of this therapeutic approach is that labeled Abs are not able to penetrate deep into solid tumors due to their large size and charge characteristics (4). In contrast, ovarian cancer cells are found mainly in the peritoneal cavity, and the disease is usually metastasized within the abdominal cavity (5). Studies have shown that intraperitoneal immuno- or radioimmunotherapy directed against the FRα can be used to treat this ailment, but these therapies are not considered mainstream treatments for this cancer. This is because the ^131^I used to label the Abs for radioimmunotherapy has a half-life of ~8 days, creates a radiation safety challenge to family and caretakers because of the high energy photons and the patients can develop human anti-mouse Abs, both with immuno- or radioimmunotherapy, thereby limiting the use of this therapeutic regimen (3, 6).

Recently, a completely human Fab fragment directed against the FRα, designated C4, was prepared by using a phage display library followed by an epitope imprinting selection. C4 was shown to have the same binding specificity as the parent Ab (7). It was hypothesized that a chemical dimer of the C4 fragment generated by molecular and chemical transformation of the Fab would be more suitable for the treatment of ovarian cancer because it would have a small size and would easily penetrate tumors (7). The Fab dimer, designated AFRA-DFM5.3, was prepared, labeled with ^131^I, and shown to accumulate primarily in the subcutaneous FR-expressing tumors in athymic mice. In another study, the label from [^131^I]-AFRA-DFM5.3 was reported to rapidly accumulate in free-floating clumps of ovarian cancer cells and solid tumors in the peritoneal cavity (8).

### Related Resource Links

FR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Folate+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Adult human FR protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_016724.2)

Human FR gene (http://www.ncbi.nlm.nih.gov/gene/2348) (Gene ID: 2348)

FR clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor+AND+targeted+AND+cancer)

FR in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/136430) database

FR pathway in Kyoto Encyclopedia of Genes and Genomes (KEGG) (http://www.genome.jp/dbget-bin/www_bget?hsa:2348+hsa:2350+hsa:2352+hsa:390243)

Folic acid information on Dailymed site (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=ff80ef4d-e04c-9f83-2b56-cccc30028f72)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22068897%5Buid%5D&cmd=DetailsSearch)]

The expression and purification of the AFRA Fab fragment from Escherichia coli and its chemical dimerization to obtain AFRA-DFM5.3 has been described by Figini et al. (7). The dimerized Fab fragment was labeled with ^131^I using a commercially available kit (with Iodogen-precoated iodination tubes), and the radiolabeling efficiency of the reaction was 86 ± 1.5% (n = 4 experiments). The labeled dimer was purified on a PD-10 desalting column and formulated in 100 mM sodium phosphate (pH 7.4), 150 mM NaCl, and 2% human serum albumin. The formulated preparation was filtered through a 0.22-μm membrane and evaluated for sterility and pyrogenicity. The radiochemical yield and radiochemical purity of the final preparation were not reported. The specific activity of the final radiolabeled product was 196 ± 25.9 MBq/mg (5.3 ± 0.7 mCi/mg; n = 4 experiments).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22068897%5Buid%5D&cmd=DetailsSearch)]

[^131^I]-AFRA-DFM5.3 was reported to have an immunoreactivity of 68 ± 5.2% (n = 4 experiments), as determined with A431FR (A431 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology) cells transfected with the FR) and OVCAR3 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-161&Template=cellBiology) cell-binding assays (7).

The labeled dimeric Fab was stable in buffer or fresh human serum for at least 24 h at 4°C or 37°C, respectively, as determined with direct binding on fixed cells and SDS-PAGE, respectively (7).

Using A431FR cells, the IC_50_ of non-radioactive AFRA-DFM5.3 was determined to be 15.3 nM (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22068897%5Buid%5D&cmd=DetailsSearch)]

The biodistribution of [^131^I]-AFRA-DFM5.3 was studied in nu/nu mice bearing subcutaneous tumors of A431FR cells (7). Control mice bore A431 cell tumors. The animals (n = 4 mice/time point) were given an intravenous injection of 1–1.5 MBq/mouse (27–40.5 μCi/mouse) ^131^I-AFRA-DFM5.3 and euthanized at various time points varying from 1 h to 24 h postinjection (p.i.) to determine the amount of label accumulated in the tumors and the major organs. Data obtained from the study were presented as percent of injected dose per gram tissue (% ID/g).

Table: Uptake of Radioactivity from [ ^ 131 ^ I]-AFRA-DFM5.3 in Tumors and Select Organs from A431 Cell (Control) or A431FR Cell Tumor-Bearing Mice. Data Obtained from Figini et al. ( 7 ).

| Control Mice (A431 Cell Tumors) | | | | A431FR Tumor-Bearing Mice
| Time post-injection (hours)
| 1 | 3 | 6 | 24 | 1 | 3 | 6 | 24
Blood (B)* | 7.27 ± 1.88 | 3.41 ± 1.42 | 1.53 ± 0.02 | 0.13 ± 0.02 | 12.37 ± 3.17 | 5.11 ± 1.53 | 2.10 ± 0.50 | 0.20 ± 0.13
Tumor (T) | 3.77 ± 0.75 | 2.84 ± 1.04 | 1.89 ± 0.64 | 0.18 ± 0.05 | 5.35 ± 2.07 | 6.29 ± 0.16 | 4.56 ± 0.01 | 1.77 ± 0.47
Kidney | 30.67 ± 4.94 | 4.01 ± 1.01 | 2.18 ± 0.35 | 0.32 ± 0.01 | 30.95 ± 4.68 | 12.69 ± 9.85 | 3.54 ± 1.77 | 0.46 ± 0.30
Liver | 3.43 ± 0.71 | 1.44 ± 0.64 | 0.72 ± 0.12 | 0.13 ± 0.01 | 6.31 ± 2.64 | 3.07 ± 1.76 | 3.54 ± 1.77 | 0.23 ± 0.19
Muscle | 1.03 ± 0.11 | 0.69 ± 0.37 | 0.36 ± 0.08 | 0.04 ± 0.03 | 1.08 ± 0.12 | 0.93 ± 0.17 | 0.39 ± 0.03 | 0.05 ± 0.01
T/B Ratio | 0.52 | 0.83 | 1.23 | 1.41 | 0.43 | 1.23 | 2.17 | 9.09

* Data presented as % ID/g.

From the above Table, it is evident that radioactivity from [^131^I]-AFRA-DFM5.3 was cleared rapidly through the urinary route of the animals. The tumor/blood radioactivity (T/B) ratio in both groups of animals increased with time, but at 6 h p.i. and 24 h p.i. the ratios in the A431FR tumor-bearing mice were approximately two-fold or six-fold higher, respectively, compared with the ratios in the control animals. No blocking studies were reported.

In another study, the uptake of radioactivity from [^131^I]-AFRA-DFM5.3 was evaluated after intraperitoneal injection of the labeled Ab dimer in nude mice bearing two different types of intraperitoneal ovarian carcinoma xenografts (from A431FR and A431MK cells, respectively) (8). Animals bearing the A431MK cell tumors served as controls for this study. Mice (n = 3–4 animals) were injected with the radiolabeled Ab dimer and euthanized at different time points (1 h p.i. to 15 h p.i.) as detailed above to obtain the various organs and the acsites fluid. The circulating half-life of [^131^I]-AFRA-DFM5.3 was longer than that of a low or non-binding control Ab ([^131^I]-AFRA-DFM6.1; circulation times were 4.4 ± 0.6 h versus 3.3 ± 0.2 h, respectively). With [^131^I]-AFRA-DFM5.3, rapid and high accumulation of radioactivity was observed in the tumor cells present in the ascites at 1 h p.i., but the solid tumors showed accumulation only after 3 h p.i. A significant difference (P < 0.0001) in the accumulation of label from [^131^I]-AFRA-DFM5.3 was apparent between the tumors of mice that developed only solid tumors and those that developed the solid tumors and/or the ascites. In animals with the ascites, the floating tumor cells showed a high uptake of the tracer compared to a very low uptake of radioactivity from the control labeled Ab (25.11 ± 6.94% ID/g versus 0.23 ± 0.05% ID/g, respectively). In addition, although [^131^I]-AFRA-DFM5.3 had a longer circulating half-life compared with the control Ab, both labeled Abs showed a similar pattern of uptake in the normal tissues or organs. No blocking studies were reported.

The efficacy of an intraperitoneal injection of [^131^I]-AFRA-DFM5.3 was evaluated for the locoregional radioimmunotherapy of animals (n = 4–8 mice) showing intraperitoneal IGROV-1 or IVCAR3 cell growth (8). All animals given the treatment had a statistically longer survival time (P = 0.0347 to <0.0001) compared to the control animals. Similar results were obtained with a single treatment of [^131^I]-AFRA-DFM5.3 independent of the dose used (37 MBq or 55 MBq/mouse (1 mCi or 1.5 mCi/mouse)). A necropsy of all animals that survived showed that the mice were tumor-free compared with control animals, which showed the presence of both the solid tumors and the ascites.

From these studies, the investigators concluded that [^131^I]-AFRA-DFM5.3 was suitable for the locoregional treatment of ovarian cancer in mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=131I-AFRA-DFM5.3%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22068897%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22068897%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Basal E., Eghbali-Fatourechi G.Z., Kalli K.R., Hartmann L.C., Goodman K.M., Goode E.L., Kamen B.A., Low P.S., Knutson K.L. (2009). Functional folate receptor alpha is elevated in the blood of ovarian cancer patients. PLoS One.
2 van Dam G.M., Themelis G., Crane L.M., Harlaar N.J., Pleijhuis R.G., Kelder W., Sarantopoulos A., de Jong J.S., Arts H.J., van der Zee A.G., Bart J., Low P.S., Ntziachristos V. (2011). Intraoperative tumor-specific fluorescence imaging in ovarian cancer by folate receptor-alpha targeting: first in-human results. Nat Med.
3 Julien D.C., Behnke S., Wang G., Murdoch G.K., Hill R.A. (2011). Utilization of monoclonal antibody-targeted nanomaterials in the treatment of cancer. MAbs.
4 Beckman R.A., Weiner L.M., Davis H.M. (2007). Antibody constructs in cancer therapy: protein engineering strategies to improve exposure in solid tumors. Cancer.
5 Lengyel E. (2010). Ovarian cancer development and metastasis. Am J Pathol.
6 Zacchetti A., Coliva A., Luison E., Seregni E., Bombardieri E., Giussani A., Figini M., Canevari S. (2009). (177)Lu- labeled MOv18 as compared to (131)I- or (90)Y-labeled MOv18 has the better therapeutic effect in eradication of alpha folate receptor-expressing tumor xenografts. Nucl Med Biol.
7 Figini M., Martin F., Ferri R., Luison E., Ripamonti E., Zacchetti A., Mortarino M., Di Cioccio V., Maurizi G., Allegretti M., Canevari S. (2009). Conversion of murine antibodies to human antibodies and their optimization for ovarian cancer therapy targeted to the folate receptor. Cancer Immunol Immunother.
8 Zacchetti A., Martin F., Luison E., Coliva A., Bombardieri E., Allegretti M., Figini M., Canevari S. (2011). Antitumor Effects of a Human Dimeric Antibody Fragment 131I-AFRA-DFM5.3 in a Mouse Model for Ovarian Cancer. J Nucl Med.